# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-synthetic HER2 specific Affibody Z_HER2:342-pep2_

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-synthetic HER2 specific Affibody Z_HER2:342-pep2_
Abbreviated name: | ^68^Ga-DOTA-Z_HER2:342-pep2_
Synonym: | ^68^Ga-ABY-002
Agent category: | Affibody, antibody fragment
Target: | Epidermal growth factor receptor (EGFR, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16); however, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of a 58-amino acid Z-domain residue from one of the IgG_1_-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <50 nM. Various radiolabeled Affibody molecules have been studied with regard to their ability for imaging HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. DOTA-Z_HER2:342-pep2_, also known as ABY-002, is a synthetic Affibody molecule that was produced for labeling with ^111^In. ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Z-DOTA111In) has been evaluated in nude mice bearing human SKOV-3 ovarian cancer cells with the use of single-photon emission computed tomography (18). Tolmachev et al. (19) prepared ^68^Ga-DOTA-Z_HER2:342-pep2_ for positron emission tomography (PET) imaging of HER2-positive tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1956))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=HER2)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342%20and%20synthesis)]

DOTA-Z_HER2:342-pep2_ (7 nmol) in ammonium acetate buffer (pH 5) was mixed with a predetermined amount of ^68^GaCl_3_ (19). DOTA/Z_HER2:342-pep2_ ratio was ~1. The mixture was incubated for 30 min at 90°C. The labeling efficiency was 98.6% of incorporation with a radiochemical purity of 98.7%. Specific activity of ^68^Ga-DOTA-Z_HER2:342-pep2_ was not mentioned. ^68^Ga-DOTA-Z_HER2:342-pep2_ was stable in ethylenediamine tetraacetic acid solution for 4 h at room temperature and in murine serum for 1 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342%20and%20in%20vitro)]

Orlova et al. (18) performed binding experiments with DOTA-Z_HER2:342-pep2_ using a Biacore sensor chip immobilized with extracellular domain of HER2 (HER2_ECD_) or chimeric HER2/Fc fusion protein (a sentence on why this second target is important?. The dissociation constants (K_d_) of DOTA-Z_HER2:342-pep2_ were calculated to be 65 pM for HER2_ECD_ and 78 pM for chimeric HER2/Fc fusion protein. The K_d_ values of His_6_-Z_HER2:342_ were 20 pM for HER2_ECD_ and 29 pM for chimeric HER2/Fc fusion protein. Therefore, the binding affinity of the synthetic Affibody molecule DOTA-Z_HER2:342-pep2_ was approximately two times lower than that of the recombinant Affibody molecule His_6_-Z_HER2:342_.

In vitro binding specificity tests showed that binding of ^68^Ga-DOTA-Z_HER2:342-pep2_ to SKOV-3 cells expressing HER2 was receptor mediated because saturation of receptors by preincubation with non-labeled His_6_-Z_HER2:342_ significantly decreased binding of ^68^Ga-DOTA-Z_HER2:342-pep2_ (P < 0.001) (19). The antigen-binding capacity of ^68^Ga-DOTA-Z_HER2:342-pep2_ was 89.4 ± 1.4%. After an initial reduction, the cell-bound radioactivity remained constant at ~73% of the initially bound activity up to 4 h when the cells were incubated with ^68^Ga-DOTA-Z_HER2:342-pep2_. At the end of 4 h, 12.4% of the radioactivity was internalized by SKOV-3 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342%20and%20rodentia)]

Tolmachev et al. (19) performed ex vivo biodistribution studies of ^68^Ga-DOTA-Z_HER2:342-pep2_ in normal mice and nude mice bearing SKOV-3 xenografts. There was a rapid renal clearance from blood in both mice. Radioactivity in the liver and gastrointestinal tract was low (~1.5% injected dose/gram (ID/g)) at 2 h after injection, whereas the radioactivity in the kidneys was very high (>200% ID/g) at 2 h after injection. The tumor radioactivity was 8.9% ID/g at 45 min and 12.4% ID/g at 2 h, and the tumor/blood ratios were 6 and 31, respectively. Pretreatment with excess Z_HER2:342_ reduced tumor accumulation by 80%_._ The radioactivity levels in the blood, lung, spleen, muscle, and bone were low at 2–3 h after injection.

PET imaging revealed that the SKOV-3 tumors and kidneys were clearly visualized in mice injected with ^68^Ga-DOTA-Z_HER2:342-pep2_ at 2 h after injection. As a comparison, ^111^In-DOTA-Z_HER2:342-pep2_ provided biodistribution data similar to those of ^68^Ga-DOTA-Z_HER2:342-pep2_.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%20342%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Orlova A., Tolmachev V., Pehrson R., Lindborg M., Tran T., Sandstrom M., Nilsson F.Y., Wennborg A., Abrahmsen L., Feldwisch J. (2007). Synthetic affibody molecules: a novel class of affinity ligands for molecular imaging of HER2-expressing malignant tumors. Cancer Res.
19 Tolmachev V., Velikyan I., Sandstrom M., Orlova A. (2010). A HER2-binding Affibody molecule labelled with 68Ga for PET imaging: direct in vivo comparison with the 111In-labelled analogue. Eur J Nucl Med Mol Imaging.